# ^111^In-Benzyl-diethylenetriaminepentaacetic acid-Z_HER2:342_

Chemical name: | ^111^In-Benzyl-diethylenetriaminepentaacetic acid-Z_HER2:342_
Abbreviated name: | ^111^In-Benzyl-DTPA-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A was constructed (17). Affibody molecules exhibit high binding affinity (K_d_) to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Z_HER2:342_ was labeled with ^111^In via isothiocyanate-benzyl-diethylenetriaminepentaacetic acid (DTPA) to form ^111^In-benzyl-DTPA-Z_HER2:342_ for single-photon emission computed tomography (SPECT) imaging in nude mice bearing human tumors (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody)]

Isothiocyanate-benzyl-DTPA and Z_HER2:342_ (1:1 molar ratio) were incubated in sodium borate buffer (pH 9) at 37°C for 20 h (18). Benzyl-DTPA-Z_HER2:342_ was isolated from the incubation mixture with a NAP-5 column. High-performance liquid chromatography-mass spectometry analysis revealed that 66% of benzyl-DTPA-Z_HER2:342_ contained one DTPA moiety, 14% had two DTPA, and 20% was unconjugated. Benzyl-DTPA-Z_HER2:342_ in 0.2 M ammonium acetate buffer (pH 5.25) was mixed with a predetermined amount of ^111^InCl_3_. The mixture was incubated at room temperature for 1 h with a labeling efficiency of >95%. ^111^In-Benzyl-DTPA-Z_HER2:342_ was purified with NAP-5 chromatography with a radiochemical purity of >98% with a specific activity of ~8 TBq/mmol (216 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20in%20vitro)]

Tolmachev et al. (18) performed binding experiments with In-benzyl-DTPA-Z_HER2:342_ using a Biacore sensor chip immobilized with extracellular domain of HER2 (HER2_ECD_). The K_d_ values of In-benzyl-DTPA-Z_HER2:342_ and Z_HER2:342_ were calculated to be 22 pM and 21 pM, respectively. In vitro binding specificity tests showed that binding of ^111^In-benzyl-DTPA-Z_HER2:342_ to SKOV-3 cells expressing HER2 was mediated by the receptors because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^111^In-benzyl-DTPA-Z_HER2:342_. The cell-bound radioactivity remained at 46–52% of the initially bound activity for up to 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20rodentia)]

Tolmachev et al. (18) performed biodistribution studies of ^111^In-benzyl-DTPA-Z_HER2:342_ (0.1 MBq (2.7 μCi)) in nude mice (n = 4/group) bearing SKOV-3 xenografts. The initial tracer accumulation in the SKOV-3 tumors was 12% injected dose per gram (ID/g) at 1 h, 12% ID/g at 4 h, 14% ID/g at 12 h, and 9% ID/g at 24 h after injection. The organ with the highest radioactivity at 1 h was the kidney (264% ID/g), followed by the lung (2.3% ID/g) and liver (2.0% ID/g). The radioactivity level in the tumors was higher than in other organs and tissues (except the kidneys) at 4–24 h. The radioactivity in the kidney was 248% ID/g at 24 h. Blood levels were 2.1% ID/g at 1 h, 0.12% ID/g at 4 h, 0.07% ID/g at 12 h, and 0.04% ID/g at 24 h. The elimination half-life of ^111^In-benzyl-DTPA-Z_HER2:342_ was 12.6 h. The biodistribution of ^111^In-benzyl-DTPA-Z_HER2:342_ was characterized by quick clearance of radioactivity from blood and all normal organs and tissues (except the kidneys). Tumor/blood ratios were 6, 100, 200, and 215 at 1, 4, 12, and 24 h after injection, respectively. Pre-administration of excess Z_HER2:342_ decreased tumor accumulation by 8.2-fold at 4 h after injection. Some inhibition was observed in the lung, liver, heart, spleen, and intestines. Positron emission tomography analysis was performed in nude mice bearing the SKOV-3 tumors after intravenous injection of 3 MBq (81 μCi) ^111^In-benzyl-DTPA-Z_HER2:342_. The tumors were clearly visualized at 4 h along with the kidneys and urinary bladder. The tumor/muscle, tumor/liver, and tumor/kidney ratios were 18, 9, and 0.1, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20affibody%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Tolmachev V., Nilsson F.Y., Widstrom C., Andersson K., Rosik D., Gedda L., Wennborg A., Orlova A. (2006). 111In-benzyl-DTPA-ZHER2:342, an affibody-based conjugate for in vivo imaging of HER2 expression in malignant tumors. J Nucl Med.